# Microbubbles conjugated with anti-matrix metalloproteinase 2 mouse monoclonal antibody sc-13595

Chemical name: | Microbubbles conjugated with anti-matrix metalloproteinase 2 mouse monoclonal antibody sc-13595
Abbreviated name: | MMP2-MBs, TMB_2_
Synonym:
Agent Category: | Antibody
Target: | Matrix metalloproteinase 2 (MMP2)
Target Category: | Enzyme
Method of detection: | Ultrasound
Source of signal / contrast: | Microbubbles (MBs)
Activation: | No
Studies: | - In vitro; - Rodents | No structure is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=matrix%20metalloproteinase%202%20microbubbles)]

Ultrasound is the most widely used imaging modality (1), and its role in noninvasive molecular imaging is expanding with ligand-carrying microbubbles (MBs) (2). MBs are composed of spherical cavities filled with a gas encapsulated in a shell. The shells are made of phospholipids, surfactant, denatured human serum albumin, or synthetic polymer. Ligands and antibodies can be incorporated into the shell surface of MBs. MBs are usually 1–8 μm in diameter, and they provide a strongly reflective interface and resonate to ultrasound waves. MBs are used as ultrasound contrast agents in imaging of inflammation, angiogenesis, intravascular thrombus, and tumors (3-5). They also have the potential to be used for drug and gene delivery (6).

Extracellular matrix (ECM) adhesion molecules consist of a complex network of fibronectins, collagens, chondroitins, laminins, glycoproteins, heparin sulfate, tenascins, and proteoglycans that surround connective tissue cells, and they are mainly secreted by fibroblasts, chondroblasts, and osteoblasts (7). Cell substrate adhesion molecules are considered essential regulators of cell migration, differentiation, and tissue integrity and remodeling. These molecules play a role in inflammation and atherogenesis, but they also participate in the process of invasion and metastasis of malignant cells in the host tissue (8). Invasive tumor cells adhere to the ECM, which provides a matrix environment for permeation of tumor cells through the basal lamina and underlying interstitial stroma of the connective tissue. Overexpression of matrix metalloproteinases (MMPs) and other proteases by tumor cells allows intravasation of tumor cells into the circulatory system after degrading the basement membrane and ECM (9).

Several families of MMPs are involved in atherogenesis, myocardial infarction, angiogenesis, and tumor invasion and metastases (10-12). MMP expression in normal cells, such as trophoblasts, osteoclasts, neutrophils, and macrophages, is highly regulated. Elevated levels of MMPs have been found in tumors associated with a poor prognosis for cancer patients (13). MMP2 is one of the major enzymes involved in the remodeling of the left ventricle after ischemia and reperfusion (I/R) in the heart (14). Su et al. (15) conjugated anti-MMP2 mouse monoclonal antibody sc-13595 to microbubbles containing polyethylene glycol (PEG) (MMP2-MBs) for contrast-enhanced ultrasound imaging of MMP2 expression in a post-I/R remodeling rat model.

### Related Resource Links:

- Chapters in MICAD (MMP (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=MMP+AND+micad%5Bbook%5D))
- Gene information in NCBI (MMP2 (http://www.ncbi.nlm.nih.gov/gene/4313))
- Articles in Online Mendelian Inheritance in Man (OMIM) (MMP2 (http://www.ncbi.nlm.nih.gov/omim/120360))
- Clinical trials (MMP (http://www.clinicaltrials.gov/ct2/results?term=matrix+metalloproteinases+))
- Drug information in FDA (MMP (http://google2.fda.gov/search?q=matrix+metalloproteinases+&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=10&y=10))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=matrix%20metalloproteinase%202%20microbubbles+synthesis)]

Su et al. (15) reported the preparation of MMP2-MBs. Hexafluoride gas was dispersed by sonication of an aqueous solution of PEG, sorbitan sterate, and Tween-80 to form a PEG contrast MB (MB_c_). MMP2 monoclonal antibody sc-13595 (~1.4 nmol) was incubated with 1 × 10^7^ MB_c_ for 10 min at 4°C. Unbounded antibody was removed from MMP2-MBs by centrifugal washings. MMP2-MBs had a mean diameter of 3.36 ± 1.61 µm. Attachment of antibody to the MB shell was confirmed with flow cytometry and microscopy. The number of antibody molecules per MB was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=matrix%20metalloproteinase%202%20microbubbles+in+vitro+studies)]

Su et al. (15) performed in vitro binding of MB_c_ and MMP2-Mbs to myocardial tissue sections from normal rats and 1-week post-I/R rats. MMP2-Mbs bound abundantly within the risk area of I/R myocardial sections with rare binding in the control area. Little binding was observed with MB_c_ in the risk area or control area. No binding was observed with MB_c_ and MMP2-MBs in the myocardial sections of control rats.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=matrix%20metalloproteinase%202%20microbubbles+rodentia)]

Su et al. (15) performed ultrasound studies of MB_c_ and MMP2-MBs binding in normal rats (n = 3/group) and 1-week post-I/R rats (n = 3/group). Myocardial contrast echocardiography was first performed to induce microvascular permeability in the heart tissue. Ultrasound was then performed at 10 min after injection of MB_c_ or MMP2-MBs (2 × 10^6^/rat). The mean myocardial video intensity in the risk area were 1.02 ± 0.19 and 1.76 ± 0.25 for MB_c_ and MMP2-MBs, respectively. The contrast enhancement of MMP2-MBs to the risk area was significantly higher than that of MB_c_ (P < 0.01). No retention of MB_c_ (1.01 ± 0.11) or MMP2-MBs (1.02 ± 0.14) was observed in the myocardial tissue of control rats. Histological and immunofluorescence staining confirmed the co-localization of MMP2-MBs to MMP2 in the risk area of 1-week post-I/R rats. No retention of MB_c_ was observed in the risk area, and no retention of MMP2-MBs was observed in the control area. No blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=matrix%20metalloproteinase%202%20microbubbles%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=matrix%20metalloproteinase%202%20microbubbles+Non+Human+Primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=matrix%20metalloproteinase%202%20microbubbles+Human+Studies)]

No references are currently available.

## References

1 Wells P.N. (2001). Physics and engineering: milestones in medicine. Med Eng Phys.
2 Liang H.D., Blomley M.J. (2003). The role of ultrasound in molecular imaging. Br J Radiol.
3 Klibanov A.L. (2005). Ligand-carrying gas-filled microbubbles: ultrasound contrast agents for targeted molecular imaging. Bioconjug Chem.
4 Lindner J.R. (2004). Microbubbles in medical imaging: current applications and future directions. Nat Rev Drug Discov.
5 Villanueva F.S., Wagner W.R., Vannan M.A., Narula J. (2004). Targeted ultrasound imaging using microbubbles. Cardiol Clin.
6 Dijkmans P.A., Juffermans L.J., Musters R.J., van Wamel A., ten Cate F.J., van Gilst W., Visser C.A., de Jong N., Kamp O. (2004). Microbubbles and ultrasound: from diagnosis to therapy. Eur J Echocardiogr.
7 Bosman F.T., Stamenkovic I. (2003). Functional structure and composition of the extracellular matrix. J Pathol.
8 Jiang W.G., Puntis M.C., Hallett M.B. (1994). Molecular and cellular basis of cancer invasion and metastasis: implications for treatment. Br J Surg.
9 Albelda S.M. (1993). Role of integrins and other cell adhesion molecules in tumor progression and metastasis. Lab Invest.
10 Berchem G., Glondu M., Gleizes M., Brouillet J.P., Vignon F., Garcia M., Liaudet-Coopman E. (2002). Cathepsin-D affects multiple tumor progression steps in vivo: proliferation, angiogenesis and apoptosis. Oncogene.
11 Brix, K., A. Dunkhorst, K. Mayer, and S. Jordans, Cysteine cathepsins: Cellular roadmap to different functions. Biochimie, 2007
12 Liu J., Sukhova G.K., Sun J.S., Xu W.H., Libby P., Shi G.P. (2004). Lysosomal cysteine proteases in atherosclerosis. Arterioscler Thromb Vasc Biol.
13 Deryugina E.I., Quigley J.P. (2006). Matrix metalloproteinases and tumor metastasis. Cancer Metastasis Rev.
14 Wang W., Schulze C.J., Suarez-Pinzon W.L., Dyck J.R., Sawicki G., Schulz R. (2002). Intracellular action of matrix metalloproteinase-2 accounts for acute myocardial ischemia and reperfusion injury. Circulation.
15 Su H., Du Y., Qian Y., Zong Y., Li J., Zhuang R., He J., Wei Z., Zhang J., Zhou X. (2011). Targeted ultrasound contrast imaging of matrix metalloproteinase-2 in ischemia-reperfusion rat model: ex vivo and in vivo studies. Mol Imaging Biol.